# ^64^Cu-{N-[1,4,8,11-Tetraazacyclotetradecanyl-1,4-phenylenebis(methylene)]-2-(aminomethyl)pyridine}

Chemical name: | ^64^Cu-{N-[1,4,8,11-Tetraazacyclotetradecanyl-1,4-phenylenebis(methylene)]-2-(aminomethyl)pyridine}
Abbreviated name: | ^64^Cu-AMD3465
Synonym:
Agent category: | Compound
Target: | Chemokine receptor 4 (CXCR4)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=64Cu%20AMD3465)]

Chemokine receptors are G-protein–coupled receptors that direct cell movement (when activated by a ligand) toward higher concentrations of chemokines. Chemokine receptor 4 (CXCR4) and its ligand, stromal cell–derived factor-1 (SDF-1 or CXCL12), are known to play a major role in the migration of progenitor cells during embryonic development of the central nervous, cardiovascular, and hematopoietic systems (1, 2). In addition, this CXCR4/SDF-1 receptor system has a function in the development, progression, and spread of various cancers (3), and the CXCR4 acts as a co-receptor for human immunodeficiency virus (HIV) on CD4^+^ T cells (4). It has also been suggested that CXCR4/SDF-1 interaction participates in the pathogenesis of neurodegenerative and inflammatory conditions (5). CXCR4 is expressed by many different types of cancers, and overexpression of CXCR4 in cancers indicates poor prognosis with aggressive and metastatic tumors and resistance to chemotherapy (6).

CXCR4 is considered to play an important role in HIV infections and cancers (4). It is critical to perform imaging studies to measure CXCR4 levels under in vivo conditions for various pathological and physiological conditions (7). ^99m^Tc-SDF-1 has been used with single-photon emission computed tomography (SPECT) to determine changes in CXCR4 expression in the heart after a myocardial infarction. ^64^Cu-1,1'-[1,4-Phenylenebis(methylene)]-bis[1,4,8,11-tetraazacyclotetradecane] (^64^Cu-AMD3100), a bicyclam inhibitor of CXCR4 activity, has been studied in mice bearing orthotopic breast tumors and in mice with lung metastases with positron emission tomography (PET) (8). {N-[1,4,8,11-Tetraazacyclotetradecanyl-1,4-phenylenebis(methylene)]-2-(aminomethyl)pyridine} (AMD3465) is a monocyclam CXCR4 inhibitor with a ~15-fold higher affinity for CXCR4 than AMD3100. De Silva et al. (9) radiolabeled AMD3465 with ^64^Cu to form ^64^Cu-AMD3465 for PET imaging of CXCR4 expression in xenograft tumors in mice.

### Related Resource Links:

- Chapters in MICAD (CXCR4 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=CXCR4+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (CXCR4 (http://www.ncbi.nlm.nih.gov/gene/7852))
- Articles in Online Mendelian Inheritance in Man (OMIM) (CXCR4 (http://www.ncbi.nlm.nih.gov/omim/162643))
- Clinical trials (CXCR4 (http://www.clinicaltrials.gov/ct2/results?term=CXCR4))
- Drug information in FDA (CXCR4 (http://google2.fda.gov/search?q=CXCR4&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=14&y=15))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=64Cu%20AMD3465%20and%20synthesis)]

AMD3465 (0.2 mg) was incubated with 370–740 MBq (10–20 mCi) ^64^CuCl_2_ in sodium acetate buffer (pH 5) for 45 min at 60°C (9). ^64^Cu-AMD3465 was purified with high-performance liquid chromatography. This procedure provided a radiochemical purity of >98% with a specific activity of 6.0 ± 3.1 GBq/µmol (162 ± 84 mCi/µmol). The log P value for ^64^Cu-AMD3465 was −2.71.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=64Cu%20AMD3465%20and%20in%20vitro)]

A receptor-binding assay was performed with ^125^I-SDF-1 (9). AMD3465 exhibited a 50% inhibition concentration (IC_50_) value of 41.7 ± 1.2 nM. Cellular accumulation was performed using human glioblastoma U87 cells transfected with human CD4 and CXCR4 (U87-stb-CXCR4, 95% of cells positive for CXCR4), U87 cells (2% positive for CXCR4) and human colon HT-29 cells (low CXCR4 expression, 30% positive for CXCR4). These cells were incubated with ^64^Cu-AMD3465 for 30 min at 4°C and then washed four times with cold binding medium. The amounts of radioactivity bound to U87-stb-CXCR4 cells, U87 cells, and HT-29 cells were 11%, 1%, and 2% incubation dose/10^6^ cells, respectively. Incubation of ^64^Cu-AMD3465 with U87-stb-CXCR4 cells at 37°C showed a linear accumulation of radioactivity with the time of incubation. At 240 min of incubation, ~50% of radioactivity was internalized. No blocking studies were performed.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=64Cu%20AMD3465%20and%20rodentia)]

De Silva et al. (9) performed ex vivo biodistribution studies of 0.74 MBq (0.020 mCi) ^64^Cu-AMD3465 in nude mice (n = 4–6/group) bearing U87-stb-CXCR4 tumor xenografts at 30, 60, 90, 240, and 600 min after injection. Tumor accumulation was 106.6 ± 6.0% injected dose/gram (ID/g), 96.3 ± 14.0% ID/g, and 51.0 ± 6.4% ID/g at 30, 90, and 240 min after injection, respectively. The maximum tumor/blood and tumor/muscle ratios of 139 and 363, respectively, occurred at 90 min after injection. Accumulation values in the liver, kidneys, bone marrow, and spleen were noticeable with 36.2% ID/g, 38.0% ID/g, 9.2% ID/g, and 4.3% ID/g, respectively, at 90 min after injection. Pretreatment with AMD3465 (25 mg/kg, 60 min before tracer injection) blocked the accumulation of ^64^Cu-AMD3465 in the tumor by >90%, whereas the accumulation in the liver, kidneys, bone marrow, and spleen was reduced by ~50% at 90 min after injection. In separate experiments, ^64^Cu-AMD3465 accumulation in U87 and HT-29 tumors was ~4% ID/g and 5.6% ID/g at 90 min after injection, respectively. Immunohistochemistry studies showed the expression of CXCR4 on tumor cells in the HT-29 tumor sections.

Biodistribution of ^64^Cu-AMD3465 was also assessed with whole-body and dynamic PET imaging in mice bearing U87-stb-CXCR4, U87, or HT-29 tumor xenografts. The accumulation in the U87-stb-CXCR4 tumors was two-fold greater than that in the kidneys and liver and ~17-fold greater than that in the U87 and HT-29 tumors. The best image contrast for U87-stb-CXCR4 tumors was observed at 90 min after injection. The liver and kidneys were also clearly visualized. Pretreatment with AMD3465 (25 mg/kg, 60 min before tracer injection) blocked the accumulation of radioactivity levels in all three tumors.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=64Cu%20AMD3465%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=64Cu%20AMD3465%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=64Cu%20AMD3465%20and%20human)]

No publication is currently available.

## NIH Support

U24 CA92871

## References

1 Juarez J., Bendall L. (2004). SDF-1 and CXCR4 in normal and malignant hematopoiesis. Histol Histopathol.
2 Miller R.J., Banisadr G., Bhattacharyya B.J. (2008). CXCR4 signaling in the regulation of stem cell migration and development. J Neuroimmunol.
3 Rubin J.B. (2009). Chemokine signaling in cancer: one hump or two?. Semin Cancer Biol.
4 Alkhatib G. (2009). The biology of CCR5 and CXCR4. Curr Opin HIV AIDS.
5 Mocchetti I., Bachis A., Masliah E. (2008). Chemokine receptors and neurotrophic factors: potential therapy against aids dementia?. J Neurosci Res.
6 Gelmini S., Mangoni M., Serio M., Romagnani P., Lazzeri E. (2008). The critical role of SDF-1/CXCR4 axis in cancer and cancer stem cells metastasis. J Endocrinol Invest.
7 Misra P., Lebeche D., Ly H., Schwarzkopf M., Diaz G., Hajjar R.J., Schecter A.D., Frangioni J.V. (2008). Quantitation of CXCR4 expression in myocardial infarction using 99mTc-labeled SDF-1alpha. J Nucl Med.
8 Nimmagadda S., Pullambhatla M., Stone K., Green G., Bhujwalla Z.M., Pomper M.G. (2010). Molecular imaging of CXCR4 receptor expression in human cancer xenografts with [64Cu]AMD3100 positron emission tomography. Cancer Res.
9 De Silva R.A., Peyre K., Pullambhatla M., Fox J.J., Pomper M.G., Nimmagadda S. (2011). Imaging CXCR4 expression in human cancer xenografts: evaluation of monocyclam 64Cu-AMD3465. J Nucl Med.